# ^64^Cu-1,4,7-Triazacyclononane-1,4,7-triacetic acid-p-isothiocyanatobenzyl-ALT-836

Chemical name: | ^64^Cu-1,4,7-Triazacyclononane-1,4,7-triacetic acid-p-isothiocyanatobenzyl-ALT-836
Abbreviated name: | ^64^Cu-NOTA-ALT-836
Synonym: | ^64^Cu-NOTA-p-Bn-SCN-ALT-836
Agent category: | Antibody
Target: | Tissue factor (TF), also known as coagulation factor III (F3), thrombokinase, or CD142
Target category: | Antigen
Method of detection: | Positron emission tomography (PET)
Source of signal\contrast: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/protein/AAA61152.1), nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/NM_001178096.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/gene/?term=2152) for more information about tissue factor.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ALT-836)]

Tissue factor (TF) is a transmembrane receptor present in subendothelial tissue, platelets, and leukocytes (1). This factor binds and localizes the coagulation factor VII to the cell surface to initiate the coagulation cascade. TF is normally expressed only in adventitial fibroblasts and vascular smooth muscle cells surrounding blood vessels, providing a hemostatic barrier that activates coagulation when the tissue is injured (2). TF can be newly synthesized upon endotoxin and cytokine stimulation of endothelial cells and leukocytes. The expression of TF is upregulated in thrombosis, tumor growth, metastasis, and angiogenesis (3, 4). There is an aberrant expression of TF in pancreatic cancer, breast cancer, glioma, leukemia, and lung cancer, with strong association of several hemostatic complications (5). ALT-836 (formerly known as Sunol-cH36) is a human/mouse chimeric monoclonal antibody (mAb) that blocks the factor X/factor IX (FX/FIX) binding site of TF and inhibits the coagulation cascade (6). This mAb has been evaluated in clinical trials (http://www.clinicaltrials.gov/ct2/results?term=ALT-836) for treatments of acute lung injury/acute respiratory distress syndrome (7). Hong et al. (8) evaluated ^64^Cu-1,4,7-triazacyclononane-1,4,7-triacetic acid-p-isothiocyanatobenzyl-ALT-836 (^64^Cu-NOTA-p-Bn-SCN-ALT-836, or ^64^Cu-NOTA-ALT-836) for positron emission tomography (PET) imaging of TF expression in nude mice bearing human pancreatic tumors with specific accumulation.

### Related Resource Links:

- Chapters in MICAD (tissue factor (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=coagulation%20factor+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (tissue factor (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2152))
- Articles in Online Mendelian Inheritance in Man (OMIM) (tissue factor (http://omim.org/entry/134390))
- Clinical trials (ALT-836 (http://www.clinicaltrials.gov/ct2/results?term=ALT-836))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ALT-836%20+synthesis)]

^64^Cu-NOTA-ALT-836 was prepared by conjugation of p-SCN-Bn-NOTA to ALT-836 in 25:1 molar ratio (8). ^64^Cu-NOTA-ALT-836 was purified with column chromatography. ^64^Cu-NOTA-ALT-836 (0.165 nmol) was radiolabeled using 37 MBq (1 mCi) ^64^CuCl_2_ in sodium acetate buffer (pH 5.0) for 30 min at 37°C. ^64^Cu-NOTA-ALT-836 was purified with PD-10 column chromatography. Total preparation time of the tracer was 70 ± 10 min (n = 6). The radiochemical yield was 79.6 ± 5.4%. The radiochemical purity was >95%. The specific activity of ^64^Cu-NOTA-ALT-836 was reported to be 180 MBq/nmol (4.86 mCi/nmol). The number of NOTA moieties per mAb conjugate was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ALT-836%20+in+vitro)]

^64^Cu-NOTA-ALT-836 exhibited immunoreactivity similar to the unconjugated mAb as determined with binding to BXPC-3 (high TF expression) and ASPC-1 (moderate TF expression) pancreatic cancer cells with flow cytometry analysis (8). Little binding was observed in PANC-1 (TF-negative) pancreatic cells. The binding levels of both mAbs to the three cell lines correlated with TF expression levels in these cells (BXPC-3 > ASPC-1 > PNAC-1).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ALT-836%20rodentia)]

PET scans were performed after intravenous injection of 5–10 MBq (135–270 μCi) ^64^Cu-NOTA-ALT-836 in nude mice (n = 4/group) bearing BXPC-3, ASPC-1, or PNAC-1 xenografts at 4, 24, and 48 h after injection (8). High radioactivity accumulation was evident in the TF-positive BXPC-3 and ASPC-1 tumors, with low accumulation in the TF-negative PNAC-1 tumors at 4, 24, and 48 h. The radioactivity levels in the BXPC-3 tumors increased from 5.7 ± 1.8% injected dose/gram (ID/g) at 4 h to 10.4 ± 0.8% ID/g at 24 h and 16.5 ± 2.6% ID/g at 48 h, whereas the radioactivity levels in the PNAC-1 tumors were 1.7 ± 0.8% ID/g, 2.8 ± 0.7% ID/g, and 2.2 ± 0.6% ID/g at 4, 24 and 48 h, respectively. Accumulation in the ASPC-1 tumors was lower than that in the BXPC-3 tumors but higher than that in the PNAC-1 tumors at all times (P < 0.05). The liver accumulation of radioactivity was 18.2 ± 1.8% ID/g, 16.7 ± 1.4% ID/g, and 10.2 ± 0.9% ID/g at 4, 24 and 48 h, respectively. The blood radioactivity was 10.6 ± 1.3% ID/g, 6.8 ± 1.5% ID/g, and 3.5 ± 0.7% ID/g at 4, 24 and 48 h, respectively. Overall, tracer accumulation in all major organs was similar among the three tumor groups. A blocking experiment was performed with mice bearing BXPC-3 tumors by administration of ALT-836 2 h before the tracer injection. Tumor accumulation was inhibited by ~80% at 4, 24 and 48 h (P < 0.05), whereas accumulation in all major organs and blood was similar between the blocking and non-blocking groups. Ex vivo biodistribution studies were performed at 48 h and showed that the radioactivity distribution patterns were similar with the PET imaging data. All major organs (such as the liver, spleen, kidney, lung, heart, and pancreas) exhibited lower radioactivity than that of the BXPC-3 tumors. Immunofluorescence staining of tumor sections confirmed the strong expression of TF in the BXPC-3 and ASPC-1 tumor cells, with weak expression in the PANC-1 tumor cells. TF staining was absent in the liver and spleen.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ALT-836%20and%20%28pig%20or%20dog%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ALT-836%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ALT-836+human)]

No publication is currently available.

## NIH Support

9U54TR000021

## References

1 Drake T.A., Morrissey J.H., Edgington T.S. (1989). Selective cellular expression of tissue factor in human tissues. Implications for disorders of hemostasis and thrombosis. Am J Pathol.
2 Nemerson Y. (1988). Tissue factor and hemostasis. Blood.
3 Fernandez P.M., Rickles F.R. (2002). Tissue factor and angiogenesis in cancer. Curr Opin Hematol.
4 Rickles F.R., Shoji M., Abe K. (2001). The role of the hemostatic system in tumor growth, metastasis, and angiogenesis: tissue factor is a bifunctional molecule capable of inducing both fibrin deposition and angiogenesis in cancer. Int J Hematol.
5 van den Berg Y.W., Osanto S., Reitsma P.H., Versteeg H.H. (2012). The relationship between tissue factor and cancer progression: insights from bench and bedside. Blood.
6 Jiao J.A., Kelly A.B., Marzec U.M., Nieves E., Acevedo J., Burkhardt M., Edwards A., Zhu X.Y., Chavaillaz P.A., Wong A., Wong J.L., Egan J.O., Taylor D., Rhode P.R., Wong H.C. (2010). Inhibition of acute vascular thrombosis in chimpanzees by an anti-human tissue factor antibody targeting the factor X binding site. Thromb Haemost.
7 Morris P.E., Steingrub J.S., Huang B.Y., Tang S., Liu P.M., Rhode P.R., Wong H.C. (2012). A phase I study evaluating the pharmacokinetics, safety and tolerability of an antibody-based tissue factor antagonist in subjects with acute lung injury or acute respiratory distress syndrome. BMC Pulm Med.
8 Hong H., Zhang Y., Nayak T.R., Engle J.W., Wong H.C., Liu B., Barnhart T.E., Cai W. (2012). Immuno-PET of Tissue Factor in Pancreatic Cancer. J Nucl Med.